# [^18^F]Fluoropropyl-Tanaproget

Chemical name: | [^18^F]Fluoropropyl-Tanaproget
Abbreviated name: | [^18^F]FPTP
Synonym:
Agent category: | Compound
Target: | Progesterone receptor (PR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTP)]

Estrogens and progesterones are endogenous hormones that produce many physiological effects (1). Estrogens act primarily by regulating gene expression. Estrogen receptors (ERs) are found in the cytoplasm and nucleus of cells in the female reproductive tract, breast, pituitary, hypothalamus, bone, liver, and other tissues, as well as in various tissues in men. Estrogens are lipophilic in that they enter the cell passively by diffusion through the cellular membrane. They bind to ERs in the cytoplasm and are transported to the nucleus.

Breast cancer is the most common malignancy in women. Approximately 33% of women who have this disease will die of disseminated breast cancer. The growth of breast epithelial cells is dependent on estrogen stimulation to induce progesterone receptor (PR) expression. Two-thirds of breast carcinomas express ERs. It has also been established that the ER status of the tumor is an important prognostic indicator in breast cancer (2). Women with ER-positive breast tumors have a better prognosis than women with ER-negative tumors in terms of responsiveness to anti-estrogen treatment. ER content in breast cancer was assessed in vitro with receptor binding assays, which suffer from inter-assay variability and are also limited by intrinsic receptor heterogeneity of the primary and metastatic tumors. 16α-[^18^F]Fluoro-17β-estradiol ([^18^F]FES) has been proven to be a valuable tracer for studies of the ER status of primary and metastatic breast cancer (3). However, [^18^F]FES is cleared from the blood and metabolized in 20 min with only 20% of [^18^F]FES intact in a study with 15 breast cancer patients (4). A newly developed nonsteroidal progestin analog, Tanaproget, exhibits a potent agonist activity for PR with a high binding affinity (K_d_ = 0.2 nM) (5). Lee et al. (6) reported the synthesis of [^18^F]fluoropropyl-Tanaproget ([^18^F]FPTP) and its tissue distribution in immature, estrogen-primed, female rats with a high uterus/blood ratio.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=estrogen%20receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Estrogen receptor (http://www.ncbi.nlm.nih.gov/gene/2099), progesterone receptor (http://www.ncbi.nlm.nih.gov/gene/5241))
- Articles in OMIM (Estrogen receptor (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=133430), progesterone receptor (http://www.ncbi.nlm.nih.gov/omim/607311))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTP%20AND%20synthesis)]

A mixture of the methanesulfonate precursor and n-Bu_4_N[^18^F]F in tert-amyl alcohol was heated for 20 min at 130ºC (6). After removal of the solvent, the mixture was heated for 10 min at 160ºC to undergo deprotection. The mixture was heated with Lawesson’s reagent in toluene for 30 min at 130ºC to convert the carbamate group to the thiocarbamate group. [^18^F]FPTP was isolated to provide a radiochemical yield of 5% (decay-corrected) with a specific activity of ~20 GBq/µmol (550 mCi/µmol) and a chemical purity of >95% after purification with high-performance liquid chromatography. The total synthesis time was ~140 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTP%20AND%20in%20vitro)]

In an alkaline phosphatase assay in T47D cells, Tanaproget had an effective dose (EC_50_) of 0.15 nM, comparable to steroidal PR agonists (e.g., medroxyprogesterone acetate (MPA, EC_50_ = 0.12 nM)) (7). Tanaproget showed high affinity for the human PR with an IC_50_ of 1.6 nM in a T47D cell cytosol competition-binding assay (IC_50_ = 10.8 nM). Tanaproget did not show any ER, androgen receptor, or glucocorticoid receptor agonist activity when tested at concentrations up to 10 μM in appropriate cell-based reporter assays. A competition binding assay was used to determine whether Tanaproget competes with [^3^H]dihydrotestosterone for sex hormone–binding globulin (SHBG) binding (8). Tanaproget did not significantly compete for the SHBG binding at a concentration up to 10 µM.

Relative binding affinities for PR were determined with a competitive binding assay using 10 nM [^3^H]R5020 ([17R-methyl-^3^H]-promegestone) as a tracer and purified full length progesterone receptor B (5). FPTP exhibited a binding affinity to PR similar to that of the parent compound Tanaproget (K_d_ = 0.2 nM).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTP%20AND%20rodentia)]

It was demonstrated that [^18^F]FPTP uptake by target tissues (the uterus and ovaries) in immature, estrogen-primed, female rats (n = 5/group) is highly specific (6). The rats were injected with 1.0 MBq (0.026 mCi) [^18^F]FPTP. The initial tracer accumulation in the uterus was 4.6 ± 1.1% injected dose per gram (ID/g) and 5.3 ± 0.4% ID/g at 1 h and 3 h after injection, respectively. Tracer accumulation in the ovaries was 2.3 ± 0.2% ID/g and 2.2 ± 0.4% ID/g at 1 h and 3 h after injection, respectively. There was also a significant reduction (~80%) of [^18^F]FPTP accumulation in the uterus and ovaries at the two time points with co-injection of excess FPTP. The accumulation in the liver, spleen, muscle, and kidneys was lower than uptake in the uterus and ovaries at 3 h after injection. The accumulation of radioactivity in the bone was 0.9% ID/g and 0.6% ID/g at 1 h and 3 h after injection, respectively. Co-injection of FPTP had little inhibitory effect in these non-targeted tissues. The uterus/blood ratios were 9 and 32 at 1 h and 3 h after injection, respectively. The ovary/blood ratios were 5 and 13 at 1 h and 3 h after injection, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTP%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTP%20AND%20primates%20not%20humans)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTP%20AND%20human)]

No publication is currently available.

## NIH Support

R01 CA025836, R24 CA086307

## References

1 Beato M., Klug J. (2000). Steroid hormone receptors: an update. Hum Reprod Update.
2 Vollenweider-Zerargui L., Barrelet L., Wong Y., Lemarchand-Beraud T., Gomez F. (1986). The predictive value of estrogen and progesterone receptors' concentrations on the clinical behavior of breast cancer in women. Clinical correlation on 547 patients. Cancer.
3 Flanagan F.L., Dehdashti F., Siegel B.A. (1998). PET in breast cancer. Semin Nucl Med.
4 Mankoff D.A., Tewson T.J., Eary J.F. (1997). Analysis of blood clearance and labeled metabolites for the estrogen receptor tracer [F-18]-16 alpha-fluoroestradiol (FES). Nucl Med Biol.
5 Zhou H.B., Lee J.H., Mayne C.G., Carlson K.E., Katzenellenbogen J.A. (2010). Imaging progesterone receptor in breast tumors: synthesis and receptor binding affinity of fluoroalkyl-substituted analogues of tanaproget. J Med Chem.
6 Lee J.H., Zhou H.B., Dence C.S., Carlson K.E., Welch M.J., Katzenellenbogen J.A. (2010). Development of [f-18]fluorine-substituted tanaproget as a progesterone receptor imaging agent for positron emission tomography. Bioconjug Chem.
7 Fensome A., Bender R., Chopra R., Cohen J., Collins M.A., Hudak V., Malakian K., Lockhead S., Olland A., Svenson K., Terefenko E.A., Unwalla R.J., Wilhelm J.M., Wolfrom S., Zhu Y., Zhang Z., Zhang P., Winneker R.C., Wrobel J. (2005). Synthesis and structure-activity relationship of novel 6-aryl-1,4-dihydrobenzo[d][1,3]oxazine-2-thiones as progesterone receptor modulators leading to the potent and selective nonsteroidal progesterone receptor agonist tanaproget. J Med Chem.
8 Zhang Z., Olland A.M., Zhu Y., Cohen J., Berrodin T., Chippari S., Appavu C., Li S., Wilhem J., Chopra R., Fensome A., Zhang P., Wrobel J., Unwalla R.J., Lyttle C.R., Winneker R.C. (2005). Molecular and pharmacological properties of a potent and selective novel nonsteroidal progesterone receptor agonist tanaproget. J Biol Chem.